# ^68^Ga-Labeled 2-[4,7-di(carboxymethyl)-1,4,7-triazonan-1-yl]-5-[(4-hydroxy-4,4-diphosphonobutyl)amino]-5-oxopentanoic acid (NOTA-bisphosphonate (BP))

Chemical name: | ^68^Ga-Labeled 2-[4,7-di(carboxymethyl)-1,4,7-triazonan-1-yl]-5-[(4-hydroxy-4,4-diphosphonobutyl)amino]-5-oxopentanoic acid (NOTA-bisphosphonate (BP))
Abbreviated name: | [^68^Ga]-NOTA-BP
Synonym: | [^68^Ga]-NOTA-bisphosphonate
Agent Category: | Compound
Target: | Bone (hydroxyapatite) at low concentration; farnesyl disphosphate (pyrophosphate) synthase (molecular target) at high concentration
Target Category: | Other (tissue); enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on above structure for information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Bisphosphonates&cmd=DetailsSearch)]

Bisphosphonates (BPs; also known as diphosphonates), such as methylene diphosphonate (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=38ac7426-d447-4327-b8c7-9e438d562865) (MDP) and zoledronic acid (http://www.pharma.us.novartis.com/product/pi/pdf/Zometa.pdf), can be labeled with technetium-99m ([^99m^Tc]-BPs) for use in bone scintigraphy to detect osteoporosis and other skeletal-related events (SREs), including bone metastases (1). These chemicals are known to promote osteoclast apoptosis and have a strong affinity for hydroxyapatite, a component of the bone matrix. The exact mechanism of action of these bone-seeking compounds is described in detail elsewhere (2-4). Although these labeled compounds have a high sensitivity, selectivity, and accuracy for the detection of SREs, they are known to generate some false positive and false negative results in the clinic (5). [^18^F]-Fluoride is another nuclide that is commonly used for bone imaging with positron emission tomography (PET) and is believed to be superior to [^99m^Tc]-BPs for the diagnosis of SREs (6); however, the main limitations of using ^18^F are the high cost of production and the requirement of a cyclotron to produce it (5). In an effort to develop an imaging compound that does not have the limitations of tracers currently used to detect SREs with scintigraphy or PET, Suzuki et al. developed a bisphosphonate labeled with ^68^Ga, which has been shown to be potentially useful for the PET imaging of the skeletal system (5).

The main advantage of using ^68^Ga (half-life = 68 min; β^+^ = 89%; E+_βmax_ = 1.9 MeV) for bone imaging over either ^99m^Tc (half-life = 6 h; γ^+^ = 100%; E+_γmax_ = 140 keV) or ^18^F (half-life = ~110 min; β^+^ = 97%; E+_βmax_ = 0.635 MeV) as a radiolabel is that ^68^Ga can be produced economically on-site with a ^68^Ge/^68^Ga generator (5). Suzuki et al. coupled a BP with 1,4,7-triazacyclononane-1,4-7-triacetic acid (NOTA-BP) and labeled the product with ^68^Ga to obtain [^68^Ga]-NOTA-BP (5). The investigators then compared the biodistribution of [^68^Ga]-NOTA-BP with that of [^99m^Tc]-methylene diphosphonate ([^99m^Tc]-MDP) and [^18^F]fluoride in rats. [^68^Ga]-NOTA-BP was also evaluated for the imaging of osteolytic bone metastasis in mice.

### Related Resource Links

Related chapters (http://www.ncbi.nlm.nih.gov/books/?term=MDP+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001037277.1) of human farnesyl diphosphate synthase

Gene information (http://www.ncbi.nlm.nih.gov/gene/2224) regarding human farnesyl diphosphate synthase (GeneID: 2224)

Farnesyl diphosphate synthase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/134629) database

Structure of farnesyl diphosphate synthase (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=59201) complexed with a bisphosphonate

Farnesyl diphosphate synthase in Kyoto Encyclopedia of Genes and Genomes (KEGG) Pathways (http://www.genome.jp/dbget-bin/www_bget?pathway+hsa00900)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=bisphosphonates) with bisphosphonates (or diphosphonates)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68ga-nota-bp%20synthesis&cmd=DetailsSearch)]

The synthesis of NOTA-BP and its labeling with ^68^Ga have been described by Suzuki et al. (5). The radiochemical purity (RCP) of the labeled product was >95% as determined with radio thin-layer chromatography (RTLC; R_f_ = 0.3–0.4). The radiochemical yield (RCY) and specific activity of the final labeled product were not reported.

[^99m^Tc]-MDP and ^18^F were obtained from commercial or academic sources, but the RCP, RCY, and specific activity of these labeled products were not mentioned (5).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68ga-nota-bp%20in%20vitro%20studies&cmd=DetailsSearch)]

Using a hydroxyapatite (HA) binding assay, the B_max_ and K_d_ of [^68^Ga]-NOTA-BP, [^99m^Tc]-MDP, and ^14^C-pamadronic acid were determined to be 14.37 nmol/mg and 0.0937 μM, 53.98 nmol/mg and 0.4898 μM, and 53.88 nmol/mg and 0.3066 μM, respectively (5). This indicated that [^68^Ga]-NOTA-BP had a higher affinity for HA than either [^99m^Tc]-MDP or ^14^C-pamadronic acid, but [^68^Ga]-NOTA-BP had a lower B_max_ than the latter two labeled compounds.

[^68^Ga]-NOTA-BP was reported to maintain a radiochemical purity of 95% (as determined with RTLC) when incubated with rat plasma for up to 3 h at 37°C (5).

The distribution of different concentrations (10 nM, 1.0 μM, and 3.7 μM) of [^68^Ga]-NOTA-BP, [^99m^Tc]-MDP, and [^18^F]fluoride in the blood cells of rats after a 30 min incubation at 37^o^ C was investigated by Suzuki et al. (5). The proportion of [^68^Ga]-NOTA-BP in the blood cells was 6.5%–8.4%, which was comparable to that of [^99m^Tc]-MDP (7.1%–10.2%) but significantly lower (P < 0.05) than that of [^18^F]fluoride (29.1%–29.7%).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68ga-nota-bp%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^68^Ga]-NOTA-BP (n = 6 animals), [^99m^Tc]-MDP (n = 7 animals), and ^18^F (n = 4 animals) was studied in normal Wistar rats as described by Suzuki et al. (5). Each rat was intravenously injected with 1.0–4.0 MBq (27–104 μCi) of the labeled compound, and the rodents were euthanized 2 h after administration to determine the amount of radioactivity accumulated in the various tissues, including the bone (tibia and fibula). Data obtained from the study were presented as percent of injected dose per gram tissue (% ID/g). The amount of radioactivity in the blood from [^68^Ga]-NOTA-BP, [^99m^Tc]-MDP, and ^18^F was 0.004 ± 0.0005% ID/g, 0.02 ± 0.005 (P < 0.05), and 0.01 ± 0.001% ID/g, respectively (P < 0.05), indicating that ^18^F was cleared rapidly from circulation compared to the other two tracers. In the muscle, the accumulation of label from [^68^Ga]-NOTA-BP, [^99m^Tc]-MDP, and ^18^F was 0.002 ± 0.0001% ID/g, 0.006 ± 0.0008% ID/g (P < 0.05), and 0.004 ± 0.0004% ID/g (P < 0.05), respectively, indicating that the accumulation of tracer from [^68^Ga]-NOTA-BP in the muscle was significantly lower than that from either [^99m^Tc]-MDP or ^18^F. The accumulation of radioactivity from [^68^Ga]-NOTA-BP, [^99m^Tc]-MDP, and ^18^F in the bone was 0.47 ± 0.21% ID/g, 0.41 ± 0.21% ID/g (P < 0.05), and 0.69 ± 0.22% ID/g (P < 0.05), respectively, showing that the uptake of ^18^F by the bone was significantly higher than that of either [^68^Ga]-NOTA-BP or [^99m^Tc]-MDP. The bone/muscle uptake (B/M) ratios for [^68^Ga]-NOTA-BP, [^99m^Tc]-MDP, and ^18^F were 2,048 ± 107, 747 ± 107 (P < 0.05), and 1,798 ± 206, respectively, showing that the B/M ratio of [^68^Ga]-NOTA-BP was superior to that of [^99m^Tc]-MDP and ^18^F.

Using severe combined immunodeficient mice with osteolytic bone metastasis (n = 3 mice), the imaging potential of [^68^Ga]-NOTA-BP was compared with that of [^99m^Tc]-MDP (5). Each animal was injected with 6.04–8.36 MBq (163–225 μCi) [^68^Ga]-NOTA-BP, and microPET images were acquired from the mice (under anesthesia) 1 h later. One day later, the same animals were injected with 18.0–19.5 MBq (489–526 μCi) [^99m^Tc]-MDP, and gamma micro-single photon emission computed tomography (SPECT) planar images were obtained from the mice (under anesthesia) at 3.0–3.25 h after injection. A high accumulation of both tracers was observed at the osteolytic lesion on the right tibia of the animals; however, microPET images obtained with [^68^Ga]-NOTA-BP showed a higher resolution than the micro-SPECT planar images acquired with [^99m^Tc]-MDP.

From these studies, the investigators concluded that [^68^Ga]-NOTA-BP can be used for the detection of osseous metastasis in mice, but further work is necessary before this agent can be used for the imaging of such lesions in humans (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68ga-nota-bp%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68ga-nota-bp%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68ga-nota-bp%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Lin J., Luo S., Chen C., Qiu L., Wang Y., Cheng W., Ye W., Xia Y. (2010). Preparation and preclinical pharmacological study on a novel bone imaging agent (99m)Tc-EMIDP. Appl Radiat Isot.
2 Kimmel D.B. (2007). Mechanism of action, pharmacokinetic and pharmacodynamic profile, and clinical applications of nitrogen-containing bisphosphonates. J Dent Res.
3 Zhang Y., Cao R., Yin F., Hudock M.P., Guo R.T., Krysiak K., Mukherjee S., Gao Y.G., Robinson H., Song Y., No J.H., Bergan K., Leon A., Cass L., Goddard A., Chang T.K., Lin F.Y., Van Beek E., Papapoulos S., Wang A.H., Kubo T., Ochi M., Mukkamala D., Oldfield E. (2009). Lipophilic bisphosphonates as dual farnesyl/geranylgeranyl diphosphate synthase inhibitors: an X-ray and NMR investigation. J Am Chem Soc.
4 Mitterhauser M., Toegel S. (2011). Radiopharmaceutical considerations on bone seeker uptake: should we learn from therapeutical targets of bisphosphonates?. Nucl Med Biol.
5 Suzuki K., Satake M., Suwada J., Oshikiri S., Ashino H., Dozono H., Hino A., Kasahara H., Minamizawa T. (2011). Synthesis and evaluation of a novel 68Ga-chelate-conjugated bisphosphonate as a bone-seeking agent for PET imaging. Nucl Med Biol.
6 Kruger S., Buck A.K., Mottaghy F.M., Hasenkamp E., Pauls S., Schumann C., Wibmer T., Merk T., Hombach V., Reske S.N. (2009). Detection of bone metastases in patients with lung cancer: 99mTc-MDP planar bone scintigraphy, 18F-fluoride PET or 18F-FDG PET/CT. Eur J Nucl Med Mol Imaging.